# Single-chain anti-epidermal growth factor receptor antibody fragment conjugated to magnetic iron oxide nanoparticles

Chemical name: | Single-chain anti-epidermal growth factor receptor antibody fragment conjugated to magnetic iron oxide nanoparticles
Abbreviated name: | ScFvEGFR-IO
Synonym:
Agent Category: | Single-chain antibody fragment (ScFv)
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Iron oxide (IO) nanoparticles
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Single+chain+anti+EGFR+antibody+conjugated+to+quantum+dots)]

The epidermal growth factor receptor (EGFR) family is a group of transmembrane glycoproteins that mediate their activity through a tyrosine kinase (TK) and regulate several normal cell functions such as growth, differentiation, proliferation, and angiogenesis (1, 2). The structure of the receptor and its various ligands are discussed elsewhere (3). A mutated EGFR or its overexpression have been correlated to various malignancies and indicate a poor therapeutic outcome for the patient (4-7). Because of its established role in the initiation, development, and metastasis of many malignant tumors, EGFR was identified as an excellent target for the treatment of cancers (8). Mishani et al. and Krause and Baumann have described various labeled monoclonal antibodies (MAbs), directed toward the extracellular (EC) domain of the EGFR because of their high target specificity, and small-molecule drugs (inhibitors directed toward the intracellular TK) that are often used alone or in combination with other drugs for the diagnosis or treatment of cancer under preclinical or clinical conditions (4, 8). However, the use of MAbs for the treatment of cancer has limitations because the large size of the molecules and long blood circulation half-lives were observed to be an impediment for their distribution within a tumor. Also, due to MAb excretion primarily through the hepatic route, radioactivity from labeled MAbs that have been used to detect cancer tends to accumulate in the liver and masks the detection of any tumors in this organ or the surrounding area (9). In addition, cancer patients treated with TK inhibitors often develop resistance to these small-molecule drugs (10). Moreover, in general, patients treated with an anti-cancer MAb or a small-molecule drug show only a modest response to the treatment (11).

In an effort to circumvent limitations observed in cancer treatment with the bulky MAbs (~160 kDa), investigators have engineered smaller (~25–30 kDa) single-chain antibody fragments (ScFv) that consist of the heavy and light variable chains of an antibody linked with a flexible peptide. The ScFv fragments are approximately five times smaller than the native MAbs, and they have been reported to have the same affinity and specificity for the target antigen as the parent MAbs (12). On the basis of the assumption that the ScFv fragments could show superior efficacy compared with the intact MAbs used for cancer therapy, investigators identified, expressed, and purified different ScFv fragments against the EGFR EC and characterized them under in vitro conditions (13, 14). Zhou et al. (14) also investigated the binding and uptake of liposomal nanoparticles (NP) bearing the ScFv fragments directed against the EGFR EC (ScFvEGFR). The liposomal ScFvEGFR were shown to bind to and be internalized by tumor cells overexpressing the EGFR.

In another study, Yang et al. conjugated the ScFvEGFR fragment to magnetic iron oxide (IO) NPs to obtain ScFvEGFR-IOs and investigated their binding and internalization by EGFR-expressing cancer cells (15). For the structure, function, and preclinical use of the IO NPs, please click here (PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=iron+oxide+nanoparticles)); for clinical evaluation of IO NP please click here (clinical trials (http://clinicaltrials.gov/ct2/show/NCT00769093?term=iron+oxide+nanoparticles&rank=1)). Using the magnetic resonance imaging (MRI) technique, the investigators demonstrated that ScFvEGFR-IOs specifically bound to and were internalized by EGFR-expressing cancer cells. In addition, the use of ScFvEGFR-IOs as a molecular imaging agent was demonstrated with MRI in an orthotopic human pancreatic cancer mouse xenograft model.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+QD+synthesis)]

The synthesis of ScFvEGFR-IOs was described by Yang et al. (15). The IO NPs were coated with amphiphilic copolymers and modified with short polyethylene glycol chains. The linking of ScFvEGFR to IO NPs was performed with 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide. The core size of the conjugated IOs was 25.4 ± 4.2 nm as determined with transmission electron microscopy and hydrodynamic light-scattering measurements. The final ScFvEGFR-IO conjugate was purified on a Nanosep 100K OMEGA filter column. The storage conditions and stability of ScFvEGFR-IOs were not reported.

Using the same technique, IO NPs conjugated to the green fluorescence protein (GFP-IO) were prepared for use as controls while performing MRI under in vitro conditions (15). On the basis of a standard curve drawn with the fluorescence obtained from different amounts of the GFP alone, ~8–10 GFP molecules were reported to be conjugated to each IO NP. The investigators assumed that the number of ScFvEGFR fragments linked to each IO NP was similar to the number of GFP molecules bound to the IO NP (15).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Yang et al. determined the specificity of ScFvEGFR-IO binding by exposing MIA PaCa-2 (human pancreatic cancer origin cells that express high levels of EGFR) and HEK293 (human embryonic kidney epithelial cells used as controls have low EGFR expression) xenograft tumor cells to ScFvEGFR-IOs and non-targeted IOs (15). The cells were then stained with Prussian blue (an iron-specific stain) and examined under the microscope. Only the MIA PaCa-2 cells showed a high level of binding of the targeted IO NP, and a few HEK293 cells showed a low level of targeted IO NP binding. In contrast, only a few MIA PaCa-2 cells were reported to bind the non-targeted IO NP, similar to the HEK293 cells.

To determine internalization of the ScFvEGFR-IOs, cultured tumor cells were exposed to either ScFvEGFR-IOs or GFP-IOs for 3 h at 37^o^ C, harvested and washed with phosphate buffered saline (pH of buffer not reported), and embedded in 1% agarose to perform MRI using a fast-spin T_2_-weighted echo imaging sequence. Several echo time data points were collected (15). A drop in the T_2_ signal intensity from ~5.6 to ~2 was reported within 150 ms only in the MIA PaCa-2 cells that were exposed to the targeted IOs. Cells exposed to GFP-IO showed a decrease from ~5.6 to ~3.75 under the same conditions, indicating that a significantly higher amount of ScFvEGFR-IO was internalized by the MIA PaCa-2 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+QD+rodentia)]

The biodistribution of ScFvEGFR-IOs was compared with that of the non-targeted IOs in nude mice bearing human pancreatic cancer cell line (MIA PaCa-2) xenograft tumors (15). The number of animals used for the two IO types in the study was not reported. The animals were injected through the tail vein with either ScFvEGFR-IOs or non-targeted IOs, and MRI was performed at different time points after the injection. Changes in the T_2_-weighted MRI signal showed that ScFvEGFR-IO accumulated primarily in the xenograft tumors from 5 to 30 h after administration of the targeted IOs. No such change was reported in tumors of mice treated with the non-targeted IOs. Using the MRI signal generated by muscle tissue as the baseline, a 4.8-fold change in the MRI signal was observed between tumors exposed to ScFvEGFR-IO and those exposed to the non-targeted IOs under in vivo conditions. To confirm observations obtained with MRI, Prussian blue staining of frozen tumors tissue sections was performed 48 h after injection of the two NP types. Tumor sections from mice treated with ScFvEGFR-IO were stained with Prussian blue, and an examination of the sections under high magnification showed that the stain was localized primarily within the cells. No such staining was evident in frozen tumor sections of mice treated with the non-targeted IOs. Compared with the muscle tissue, the relative contrast intensities of the liver, spleen, kidneys, and brain were ~0.6, 0.5, ~0.02, and <0.01, respectively, at 28 h after injection of the non-targeted IOs. The relative contrast intensities for these organs were 0.5, ~0.35, ~0.02, and ~0.05, respectively, at 28 h after injection of the targeted IOs. With results obtained from various studies, the investigators concluded that the ScFvEGFR-conjugated IO NPs could be detected with MRI in EGFR-expressing tumors under in vivo conditions.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+IO+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+IO+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+IO+Human+Studies)]

No references are currently available.

## Supplemental Information

### NIH Support

Some of the studies reported in this chapter were funded by NIH Grants P50-CA58207 and CA119338-01.

### References

1 Huang Z., Brdlik C., Jin P., Shepard H.M. (2009). A pan-HER approach for cancer therapy: background, current status and future development. Expert Opin Biol Ther.
2 Diagaradjane P., Orenstein-Cardona J.M., Colon-Casasnovas N.E., Deorukhkar A., Shentu S., Kuno N., Schwartz D.L., Gelovani J.G., Krishnan S. (2008). Imaging epidermal growth factor receptor expression in vivo: pharmacokinetic and biodistribution characterization of a bioconjugated quantum dot nanoprobe. Clin Cancer Res.
3 Schneider M.R., Wolf E. (2009). The epidermal growth factor receptor ligands at a glance. J Cell Physiol.
4 Mishani E., Abourbeh G., Eiblmaier M., Anderson C.J. (2008). Imaging of EGFR and EGFR tyrosine kinase overexpression in tumors by nuclear medicine modalities. Curr Pharm Des.
5 Lievre A., Bachet J.B., Le Corre D., Boige V., Landi B., Emile J.F., Cote J.F., Tomasic G., Penna C., Ducreux M., Rougier P., Penault-Llorca F., Laurent-Puig P. (2006). KRAS mutation status is predictive of response to cetuximab therapy in colorectal cancer. Cancer Res.
6 Ke S., Wen X., Gurfinkel M., Charnsangavej C., Wallace S., Sevick-Muraca E.M., Li C. (2003). Near-infrared optical imaging of epidermal growth factor receptor in breast cancer xenografts. Cancer Res.
7 Charpidou A., Blatza D., Anagnostou E., Syrigos K.N. (2008). Review. EGFR mutations in non-small cell lung cancer--clinical implications. In Vivo.
8 Krause M., Baumann M. (2008). Clinical biomarkers of kinase activity: examples from EGFR inhibition trials. Cancer Metastasis Rev.
9 Pantaleo, M.A., M. Nannini, A. Maleddu, S. Fanti, C. Nanni, S. Boschi, F. Lodi, G. Nicoletti, L. Landuzzi, P.L. Lollini, and G. Biasco, Experimental results and related clinical implications of PET detection of epidermal growth factor receptor (EGFr) in cancer. Ann Oncol, 2008
10 Engelman J.A., Settleman J. (2008). Acquired resistance to tyrosine kinase inhibitors during cancer therapy. Curr Opin Genet Dev.
11 Vogel C.L., Cobleigh M.A., Tripathy D., Gutheil J.C., Harris L.N., Fehrenbacher L., Slamon D.J., Murphy M., Novotny W.F., Burchmore M., Shak S., Stewart S.J., Press M. (2002). Efficacy and safety of trastuzumab as a single agent in first-line treatment of HER2-overexpressing metastatic breast cancer. J Clin Oncol.
12 Honegger, A., Engineering antibodies for stability and efficient folding. Handb Exp Pharmacol, 2008(181): p. 47-68.
13 Horak E., Heitner T., Robinson M.K., Simmons H.H., Garrison J., Russeva M., Furmanova P., Lou J., Zhou Y., Yuan Q.A., Weiner L.M., Adams G.P., Marks J.D. (2005). Isolation of scFvs to in vitro produced extracellular domains of EGFR family members. Cancer Biother Radiopharm.
14 Zhou Y., Drummond D.C., Zou H., Hayes M.E., Adams G.P., Kirpotin D.B., Marks J.D. (2007). Impact of single-chain Fv antibody fragment affinity on nanoparticle targeting of epidermal growth factor receptor-expressing tumor cells. J Mol Biol.
15 Yang L., Mao H., Wang Y.A., Cao Z., Peng X., Wang X., Duan H., Ni C., Yuan Q., Adams G., Smith M.Q., Wood W.C., Gao X., Nie S. (2008). Single Chain Epidermal Growth Factor Receptor Antibody Conjugated Nanoparticles for in vivo Tumor Targeting and Imaging. Small.